# ^68^Ga-1,4,7-Triazacyclononane-1,4-diacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1.4-diacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Various BBN analogs has been label with ^99m^Tc and ^111^In for single-photon emission computed tomography imaging studies (7) and ^64^Cu, ^68^Ga, and ^86^Y for positron emission tomography imaging studies (8, 9). Dijkgraaf et al. (10) 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling 8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (8-Aoc-BBN[7-14]NH_2_) with ^68^Ga. ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ was evaluated as a PET imaging agent of GRPR in nude mice bearing human PC-3 prostate cancer cells.

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(GRPR%20OR%20GRP-R)%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), bombesin (http://www.ncbi.nlm.nih.gov/books?term=bombesin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/gene/2925), GRP (http://www.ncbi.nlm.nih.gov/gene/2922))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670), GRP (http://omim.org/entry/137260))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=bombesin))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+synthesis)]

8-Aoc-BBN[7-14]NH_2_ was prepared with solid-phase peptide synthesis with subsequent addition of NOTA group to form NOTA-8-Aoc-BBN[7-14]NH_2_ (10). ^68^GaCl_3_ was added to a solution of NOTA-8-Aoc-BBN[7-14]NH_2_ in sodium acetate buffer (pH 4.1). The mixture was heated for 10 min at 95°C. The product, ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_, was purified with cartridge chromatography with 50-90% yield and a radiochemical purity of >95%. The specific activity of ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ was >10 MBq/nmol (0.27 mCi/nmol) at the end of synthesis. Total preparation time was ~45 min. ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ exhibited a Log P value of -1.98 ± 0.03.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+in+vitro)]

Dijkgraaf et al. (10) performed in vitro inhibition studies of NOTA-8-Aoc-BBN[7-14]NH_2_ and ^nat^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ in cultured human prostate PC-3 tumor cells with ^111^In-NOTA-8-Aoc-BBN[7-14]NH_2_. The 50% inhibition concentration (IC_50_) values for NOTA-8-Aoc-BBN[7-14]NH_2_ and ^nat^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ were 0.37 ± 0.15 nM and 0.41 ± 0.15 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+%20rodentia)]

Dijkgraaf et al. (10) performed ex vivo biodistribution studies of ^68^Ga-NOTA-8-Aoc-BBN[7-14]NH_2_ (~0.3 nmol) in nude mice bearing PC-3 xenografts with (n = 6) or without (n = 3) coinjection of 100-fold excess unlabeled NOTA-8-Aoc-BBN[7-14]NH_2_ at 1 h after injection. Tumor accumulation was 1.24 ± 0.26% injected dose per gram (ID/g). The organ with the highest accumulation was the pancreas (6% ID/g), followed by the colon (1% ID/g), small intestine (2% ID/g), liver (1% ID/g), kidney (1% ID/g), and stomach (0.5% ID/g). Little accumulation was observed in the spleen, lung, blood and muscle (<0.5% ID/g). NOTA-8-Aoc-BBN[7-14]NH_2_ blocked tumor accumulation by 83%. Significant inhibition (>90%) was also observed in the pancreas, stomach and colon. PET imaging studies were not performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Varvarigou A., Bouziotis P., Zikos C., Scopinaro F., De Vincentis G. (2004). Gastrin-releasing peptide (GRP) analogues for cancer imaging. Cancer Biother Radiopharm.
8 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
9 Schuhmacher J., Zhang H., Doll J., Macke H.R., Matys R., Hauser H., Henze M., Haberkorn U., Eisenhut M. (2005). GRP receptor-targeted PET of a rat pancreas carcinoma xenograft in nude mice with a 68Ga-labeled bombesin(6-14) analog. J Nucl Med.
10 Dijkgraaf I., Franssen G.M., McBride W.J., D'Souza C.A., Laverman P., Smith C.J., Goldenberg D.M., Oyen W.J., Boerman O.C. (2012). PET of Tumors Expressing Gastrin-Releasing Peptide Receptor with an 18F-Labeled Bombesin Analog. J Nucl Med.